# 4-[^18^F]Fluorobenzoyl-Phe-Ala-Leu-Gly-Glu-Ala-NH_2_

Chemical name: | 4-[^18^F]Fluorobenzoyl-Phe-Ala-Leu-Gly-Glu-Ala-NH_2_
Abbreviated name: | [^18^F]FBA-FALGEA-NH_2_
Synonym: | [^18^F]FB-FALGEA-NH_2_
Agent Category: | Peptide
Target: | Epidermal growth factor receptor variant III (EGFRvIII)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FALGEA&cmd=DetailsSearch)]

Epidermal growth factor (EGF) is a 53-amino-acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain (2, 3). EGFR, which is overexpressed in many malignant epithelial tumors, contributes to gene amplification, which is believed to introduce mutations in the receptor (4). The overexpression, amplification, and/or mutation of EGFR can lead to the development of cancer. The most common mutation observed in the receptor is the deletion of a segment (amino acid residues 6–273 of the EGFR extracellular domain), including the ligand-binding region, which results in the generation of a variant known as constitutively activated variant III EGFR (EGFRvIII) (5). Although EGFRvIII is nonresponsive to EGF, it remains a constantly operating downstream tyrosine kinase signaling pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (6). EGFRvIII has not been identified in normal tissues.

Monoclonal antibody (mAb) 806 and chimeric antibody ch806 (7, 8), which specifically target EGFRvIII, were radiolabeled for imaging EGFRvIII expression in tumors. However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging because of poor tissue and tumor penetration (9). Smaller antibody fragments and peptides have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Denholt et al. (10) identified an EGFRvIII-targeting peptide, H-Phe-Ala-Leu-Gly-Glu-Ala-NH_2_ (H-FALGEA-NH_2_) using a Positional Scanning Synthetic Combinatorial Library. H-FALGEA-NH_2_ was labeled with 4-[^18^F]fluorobenzoic acid ([^18^F]FBA) to form [^18^F]FBA-FALGEA-NH_2_ (11). [^18^F]FBA-FALGEA-NH_2_ has been evaluated for imaging of EGFRvIII expression in human glioblastoma multiforme (GBM) tumors in nude mice using positron emission tomography (PET).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), EGFRvIII (http://www.ncbi.nlm.nih.gov/books?term=EGFRvIII%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (EGFRvIII (http://www.clinicaltrials.gov/ct2/results?term=EGFRvIII))
- Drug information in FDA (EGFRvIII (http://google2.fda.gov/search?q=EGFRvIII&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FALGEA%20synthesis&cmd=DetailsSearch)]

[^18^F]FBA was synthesized in two steps from [^18^F]KF (Kryptofix 2.2.2./K_2_CO_3_) (11). The decay-corrected yields of [^18^F]FBA were 22%–54%, based on starting with [^18^F]KF. H-FALGEA-XAL-resin and 250–500 MBq (6.8–13.5 mCi) [^18^F]FBA were incubated for 30 min at room temperature. [^18^F]FBA-FALGEA-NH_2_ was cleaved from the resin by heating with trifluoroacetic acid for 20 min at 35°C. Total synthesis time was ~180 min, including the final high-performance liquid chromatography (HPLC) purification. The decay-corrected radiochemical yields, radiochemical purity, and specific activity of [^18^F]FBA-FALGEA-NH_2_ were 7.3 ± 1.1%, 95 ± 3%, and 6.4 ± 1.1 GBq/µmol (170 ± 30 mCi/µmol) (n = 6), respectively, at the end of HPLC purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FALGEA%20in%20vitro&cmd=DetailsSearch)]

The binding affinity (K_d_) values of [^18^F]FBA-FALGEA-NH_2_ to NR6M cells (expressing EGFRvIII) and NR6W-A cells (expressing EGFR) were reported to be 23 nM and 691 nM (11), respectively. The B_max_ (receptor density) values for EGFRvIII and EGFR were reported to be 77 pmol × 10^3^ cells and 596 nmol × 10^3^ cells, respectively. The in vitro stability of [^18^F]FBA-FALGEA-NH_2_ in nude mouse plasma was 85% and 53% intact after 30 min and 60 min of incubation, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FALGEA%20rodentia&cmd=DetailsSearch)]

Denholt et al. (11) performed PET imaging studies in nude mice bearing EGFRvIII-expressing human GBM tumors (7 mice, 11 tumors) and nude mice bearing EGFRvIII non-expressing human GBM tumors (5 mice, 10 tumors) at 60 min after injection of 5.7 ± 2.5 MBq (0.15 ± 0.7 mCi) [^18^F]FBA-FALGEA-NH_2_. The EGFRvIII-positive tumors were clearly visualized compared to the control tumors. The tumor/muscle ratios for EGFRvIII-positive tumors and control tumors were 7.8 ± 3.2 and 3.4 ± 1.0, respectively. The average standard uptake value (SUV = Tissue concentration/(injected dose/body weight)) of 0.11 was low for the EGFRvIII-positive tumors. The liver and kidneys were also visualized in both groups of tumor-bearing mice with higher radioactivity in the kidneys. There was a linear correlation between tumor/muscle ratios and EGFRvIII mRNA expression on the tumors (R = 0.86, P < 0.007). No blocking studies were performed. Furthermore, no intact [^18^F]FBA-FALGEA-NH_2_ was detected in the plasma at 5 min after injection, indicating rapid metabolism by blood peptidases. In comparison, [^18^F]FDG PET studies were performed one day before [^18^F]FBA-FALGEA-NH_2_ PET studies in the same nude mice bearing EGFRvIII tumors. The tumor/muscle ratio was 2.6 with an average SUV of 0.54 at 60 min after injection. The investigators concluded that a more stable peptide with higher affinity for EGFRvIII is needed to decrease the large variation in binding of [^18^F]FBA-FALGEA-NH_2_ to EGFRvIII-positive tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FALGEA%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FALGEA%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FALGEA%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
3 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 McGregor D.P. (2008). Discovering and improving novel peptide therapeutics. Curr Opin Pharmacol.
10 Denholt C.L., Hansen P.R., Pedersen N., Poulsen H.S., Gillings N., Kjaer A. (2009). Identification of novel peptide ligands for the cancer-specific receptor mutation EFGRvIII using a mixture-based synthetic combinatorial library. Biopolymers.
11 Denholt C.L., Binderup T., Stockhausen M.T., Poulsen H.S., Spang-Thomsen M., Hansen P.R., Gillings N., Kjaer A. (2011). Evaluation of 4-[18F]fluorobenzoyl-FALGEA-NH2 as a positron emission tomography tracer for epidermal growth factor receptor mutation variant III imaging in cancer. Nucl Med Biol.